# 9-(4-(2-[^18^F]Fluoroethyl)benzyl)-9-azabicyclo[3.3.1]nonan-3-yl-2-methoxy-5-methyl-phenylcarbamate

Chemical name: | 9-(4-(2-[^18^F]Fluoroethyl)benzyl)-9-azabicyclo[3.3.1]nonan-3-yl-2-methoxy-5-methyl-phenylcarbamate
Abbreviated name: | [^18^F]WC-59
Synonym:
Agent Category: | Compound
Target: | Sigma 2 receptors
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^18^F]WC-59 for additional information regarding the compound in PubChem (http://pubchem.ncbi.nlm.nih.gov/). Click on gene (http://www.ncbi.nlm.nih.gov/gene/10280?ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_147157.1?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) or protein (http://www.ncbi.nlm.nih.gov/protein/NP_671513.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) for information regarding the human sigma receptor.

## Background

[PubMed] (http://www.ncbi.nlm.nih.gov/pubmed?term=sigma%202%20receptor&cmd=DetailsSearch)

Sigma receptors (SR) are known to exist as subtypes 1 (Sig-1R) and 2 (Sig-2R) and are found in the central nervous system and the peripheral tissues. Both receptor subtypes have a different distribution in the two types of tissues, and the exact biological function of these receptors is not known (1). Of the two receptor subtypes, only the Sig-1R has been cloned, expressed, and purified (2). The Sig-2R is known to be overexpressed in various malignant tumors and to promote cell proliferation, indicating that these receptors may play a role in the development of some cancers and could be targeted for the development of different anti-cancer drugs or imaging agents for tumors that overexpress Sig-2R (3). Several clinical trials (http://clinicaltrials.gov/ct2/results?term=sigma+2+receptor) have been approved by the United States Food and Drug Administration for the evaluation of drugs that target the Sig-2R for the imaging and treatment of different clinical conditions. In addition, Sig-2R ligands have been used in preclinical studies to chemosensitize (http://mct.aacrjournals.org/content/2/8/805.full.pdf+html) tumors to low doses of anti-cancer drugs that are otherwise toxic when given at high doses to animals bearing mammalian cell line tumors (4, 5).

Investigators have developed and characterized several SR ligands, but most of them are either selective only for the Sig-1R or have similar affinity for both the SR subtypes, therefore limiting their use as anti-cancer or Sig-2R imaging agents (5). In an effort to develop a Sig-2R ligand with high specificity, Chu et al. (5) developed several analogs of 9-benzyl-9-azabicyclo[3.3.1]nonan-3-yl-2-methoxy-5-methylphenylcarbamate, which has been shown previously to have a high binding selectivity for Sig-2R. Among these analogs, 9-(4-(2-fluoroethyl)benzyl)-9-azabicyclo[3.3.1]nonan-3-yl-2-methoxy-5-methyl-phenylcarbamate (designated WC-59) was shown to be a potent Sig-2R ligand under in vitro conditions. WC-59 was subsequently labeled with ^18^F to obtain [^18^F]WC-59 and characterized under in vitro conditions. Biodistribution of the labeled compound was also studied in mice bearing murine EMT-6 cell tumors that express the Sig-2R.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-WC%2059%20synthesis&cmd=DetailsSearch)]

The synthesis and ^18^F labeling of WC-59 was described by Chu et al. (5). The total time required for the synthesis and purification of [^18^F]WC-59 was reported to be 100 min with a decay-corrected radiochemical yield of ~15%. The radiochemical purity of the tracer was >99.9%, and the specific activity at the end of synthesis was 155.4 GBq/μmol (4.2 Ci/μmol). The stability and storage conditions of the labeled compound were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-WC%2059%20in%20vitro%20studies&cmd=DetailsSearch)]

The binding affinity values of WC-59 for the Sig-1R and Sig-2R were reported to be 1,710.5 ± 84.0 and 0.82 ± 0.13 nM, respectively, with a Sig-1R/Sig-2R ratio of 2,087 (5) as determined with competitive inhibition studies described elsewhere (6).

To evaluate the use of [^18^F]WC-59 as an imaging agent for solid tumors expressing Sig-2R, receptor binding of the tracer was studied using cell membranes isolated from mouse breast tumors derived from EMT-6 cells (5). The density of Slg-2R on the tumor cells was reported to be ~3,700 fmol/mg protein, and the receptor affinity of the labeled compound was determined to be ~2 nM.

From these studies the investigators concluded that [^18^F]WC-59 could be evaluated as an imaging agent for solid tumors expressing Sig-2R (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-WC%2059%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]WC-59 was studied in BALB/c mice bearing murine EMT-6 cell tumors (5). The radiolabel was administered to the animals through the tail vein, and the mice were euthanized at preselected time points up to 2 h after treatment (the number of animals used per time point was not reported). Blood, tumors, and major organs were harvested from the animals to determine the amount of radioactivity accumulated in the various tissues. Data were presented as percentage uptake of injected dose per gram tissue (% ID/g). Radioactivity was rapidly taken up by the lungs, heart, kidneys, liver, and muscles (111.00 ± 13.52, 18.49 ± 2.50, 22.42 ± 2.91, 21.14 ± 3.59, and 4.60 ± 0.76% ID/g, respectively, at 5 min postinjection), and most of it was lost from the lungs, heart, kidneys, and muscles (4.98 ± 0.27, 1.22 ± 0.18, 5.82 ± 0.33, and 1.62 ± 0.27% ID/g, respectively) by 2 h after treatment, with the exception of the liver (17.11 ± 1.57% ID/g). The tumors had an accumulation of 1.39 ± 0.34% ID/g at 5 min, and it increased to 4.08 ± 0.66% ID/g at 2 h after treatment. The tumor/blood, tumor/muscle, tumor/fat, and tumor/lung ratios were 6.96, 2.53, 0.32, and 0.82, respectively, at 2 h after injection. From these ratios the investigators concluded that, compared with the ^18^F-labeled ligands available for the Sig-2R (7), [^18^F]WC-59 was not a superior ligand for the detection and determination of the proliferation potential of tumor cells expressing this receptor. No blocking studies were reported. Subtype specificity under in vivo conditions was assumed from the in vitro data.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-WC%2059%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-WC%2059%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Some studies presented in this chapter were supported by a National Institutes of Health grant CA 102869.

## References

1 Collier T.L., Waterhouse R.N., Kassiou M. (2007). Imaging sigma receptors: applications in drug development. Curr Pharm Des.
2 Hanner M., Moebius F.F., Flandorfer A., Knaus H.G., Striessnig J., Kempner E., Glossmann H. (1996). Purification, molecular cloning, and expression of the mammalian sigma1-binding site. Proc Natl Acad Sci U S A.
3 Hashimoto K., Ishiwata K. (2006). Sigma receptor ligands: possible application as therapeutic drugs and as radiopharmaceuticals. Curr Pharm Des.
4 Kashiwagi H., McDunn J.E., Simon P.O., Goedegebuure P.S., Vangveravong S., Chang K., Hotchkiss R.S., Mach R.H., Hawkins W.G. (2009). Sigma-2 receptor ligands potentiate conventional chemotherapies and improve survival in models of pancreatic adenocarcinoma. J Transl Med.
5 Chu W., Xu J., Zhou D., Zhang F., Jones L.A., Wheeler K.T., Mach R.H. (2009). New N-substituted 9-azabicyclo[3.3.1]nonan-3alpha-yl phenylcarbamate analogs as sigma2 receptor ligands: synthesis, in vitro characterization, and evaluation as PET imaging and chemosensitization agents. Bioorg Med Chem.
6 Xu J., Tu Z., Jones L.A., Vangveravong S., Wheeler K.T., Mach R.H. (2005). [3H]N-[4-(3,4-dihydro-6,7-dimethoxyisoquinolin-2(1H)-yl)butyl]-2-methoxy-5 -methylbenzamide: a novel sigma-2 receptor probe. Eur J Pharmacol.
7 Tu Z., Xu J., Jones L.A., Li S., Dumstorff C., Vangveravong S., Chen D.L., Wheeler K.T., Welch M.J., Mach R.H. (2007). Fluorine-18-labeled benzamide analogues for imaging the sigma2 receptor status of solid tumors with positron emission tomography. J Med Chem.